# Manganese(II)-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-G3 nanoglobule-CGLIIQKNEC (CLT1)

Chemical name: | Manganese(II)-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-G3 nanoglobule-CGLIIQKNEC (CLT1)
Abbreviated name: | Mn-DOTA-G3-CLT1
Synonym: | P-G3-Mn
Agent category: | Peptide
Target: | Fibrin-fibronectin clot complexes
Target category: | Acceptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Manganese, Mn
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal, and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide nanoparticles and other iron oxide formulations affect T2 primarily and lead to decreased signals. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

Extracellular matrix adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (2). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (3). A meshwork of clotted plasma protein was present in the tumor stroma but not in normal tissues, providing a functional matrix for angiogenesis, cell migration, and tumor cell invasion (4). There are high levels of collagens, fibronectin, and fibrin in the tumor connective tissues.

Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (5, 6). Gd-Labeled diethylenetriamine pentaacetic acid (Gd-DTPA) was the first intravenous MRI contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical use. However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their use as imaging agents in the vasculature and cancer. Furthermore, they are largely nonspecific. CGLIIQKNEC (CLT1), a fibronectin-fibrin binding cyclic peptide, was identified with phage display screening (4). The peptide was conjugated with Gd-DTPA to form Gd-DTPA-CLT1 for imaging of fibronectin-fibrin complexes in tumor tissues showing specific accumulation in the tumors (7). Tan et al. (8) prepared a CLT1-targeted contrast agent (Gd-DOTA-G3-CLT1) with Gd-tetraazacyclododecane-1,4,7,10-tetraacetic acid (GD-DOTA)_43_ monoamide chelates and three CLT1 molecules conjugated to a generation 3 (G3) polylysine dendrimer with a cubic silsesquioxane core. Gd-DOTA-G3-CLT1 was evaluated as a MRI tumor contrast agent in nude mice bearing MDA-MB-231 human breast carcinoma xenografts. However, Gd^3+^ may lead to renal toxicity in patients. Mn^2+^ ion is a cofactor for enzymes and receptors, and Mn-based agents should have lower side effects than those of Gd-based agents (9). Tan et al. (10) evaluated Mn-DOTA-G3-CLT1 as a MRI tumor contrast agent in nude mice bearing MDA-MB-231 human breast carcinoma xenografts.

### Related Resource Links:

- Chapters in MICAD (CLT1 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=CLT1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (fibrinogen (http://www.ncbi.nlm.nih.gov/gene/2243), fibronectin (http://www.ncbi.nlm.nih.gov/gene/2335))
- Articles in Online Mendelian Inheritance in Man (OMIM) (fibrinogen (http://www.ncbi.nlm.nih.gov/omim/134820), fibronectin (http://omim.org/entry/135600))
- Clinical trials (Gd-DTPA (http://www.clinicaltrials.gov/ct2/results?term=Gd-DTPA), Gd-DOTA (http://www.clinicaltrials.gov/ct2/results?term=Gd-DOTA))
- Drug information in FDA (Gd-DTPA (http://google2.fda.gov/search?q=Gd-DTPA&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1), Gd-DOTA (http://google2.fda.gov/search?q=Gd-DOTA&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+synthesis)]

CLT1 conjugate with polyethylene glycol (PEG)-propargyl group at the N-terminus was synthesized using solid-phase peptide synthesis (8). G3 nanoglobules were synthesized as previously described (11). G3 nanoglobules (diameter: 3.7 nm) were activated with azido-dPEG N-hydroxysuccinimide for CTL1 conjugation and DOTA-tris(t-Bu) for Mn^2+^ labeling. The G3 nanoglobule-(DOTA)_42_-(PEG-azido)_4_ conjugate was prepared with 82% yield, and its molecular weight was confirmed with mass spectroscopy. The G3 nanoglobule-(DOTA)_42_-(PEG-azido)_4_ conjugate (1.48 µmol) was incubated with four-fold excess of Mn(OAc)_2_ in ammonium acetate solution for 50 min at 100ºC, with 97% yield. The product, G3 nanoglobule-(Mn-DOTA)_42_-(PEG-azido)_4_ conjugate, was purified with dialysis. The G3 nanoglobule-(Mn-DOTA)_42_-(PEG-azido)_4_ conjugate (1.43 µmol), copper(II) sulfate (4 µmol), and CTL1-PEG-propargyl conjugate (8.58 µmol) were incubated for 24 h at room temperature. The final product, G3 nanoglobule-(Mn-DOTA)_42_-(CTL1)_2_ (Mn-DOTA-G3-CLT1) conjugate, was purified with ultrafiltration and dialysis with 80% yield, and its molecular weight was confirmed with mass spectroscopy. There were 42 Mn and 2 CTL1 moieties per G3 nanoglobule.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+in+vitro)]

Mn-DOTA-G3-CLT1 exhibited r_1_ and r_2_ values of 3.13 mM^–1^s^–1^ per Mn and 8.74 mM^–1^s^–1^ per Mn at 3 T, respectively (10). Mn-DOTA-G3-CLT1 had a size of 5.2 nm as measured with dynamic laser scattering. Non-targeted Mn-DOTA-G3 exhibited r_1_ and r_2_ values of 2.84 mM^–1^s^–1^ per Mn and 12.61 mM^–1^s^–1^ per Mn at 3 T, respectively. Mn-DOTA-G3 had a size of 4.2 nm. Mn-DOTA-G3-CLT1 exhibited a relatively large stability constant against transmetalation (log K_MnL_ = 20.2) as compared with Mn-DTPA (log K_MnL_ = 15.6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+rodentia)]

Tan et al. (10) performed dynamic T1-weighted MRI (7 T) studies in female nude mice (n = 3) bearing MDA-MB-231 xenografts with intravenous injection of 0.03 mmol Mn/kg Mn-DOTA-G3-CLT1. Mn-DOTA-G3 (0.03 mmol Mn/kg) was used a control contrast agent. Contrast-enhanced MRI images were obtained before injection and at 2, 5, 10, 15, 20, and 25 min after injection. Enhanced contrast in the tumor tissues was visualized for Mn-DOTA-G3-CLT1 at 2–25 min after injection. Contrast/noise ratio (CNR) for Mn-DOTA-G3-CLT1 was ~140% higher than the non-targeted agent (Mn-DOTA-G3) at 2–25 min (P < 0.05). Little enhancement was observed in the myocardium and liver for both agents. On the other hand, strong enhancement was observed in the urinary bladder over time with both agents, which were readily excreted through glomerular filtration because of their small sizes (<6 nm). No blocking and ex vivo biodistribution studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+human)]

No publication is currently available.

## NIH Support

R01 CA097465

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
3 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
4 Pilch J., Brown D.M., Komatsu M., Jarvinen T.A., Yang M., Peters D., Hoffman R.M., Ruoslahti E. (2006). Peptides selected for binding to clotted plasma accumulate in tumor stroma and wounds. Proc Natl Acad Sci U S A.
5 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
6 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
7 Ye F., Wu X., Jeong E.K., Jia Z., Yang T., Parker D., Lu Z.R. (2008). A peptide targeted contrast agent specific to fibrin-fibronectin complexes for cancer molecular imaging with MRI. Bioconjug Chem.
8 Tan M., Wu X., Jeong E.K., Chen Q., Lu Z.R. (2010). Peptide-targeted Nanoglobular Gd-DOTA monoamide conjugates for magnetic resonance cancer molecular imaging. Biomacromolecules.
9 Crossgrove J., Zheng W. (2004). Manganese toxicity upon overexposure. NMR Biomed.
10 Tan M., Wu X., Jeong E.K., Chen Q., Parker D.L., Lu Z.R. (2010). An effective targeted nanoglobular manganese(II) chelate conjugate for magnetic resonance molecular imaging of tumor extracellular matrix. Mol Pharm.
11 Kaneshiro T.L., Jeong E.K., Morrell G., Parker D.L., Lu Z.R. (2008). Synthesis and evaluation of globular Gd-DOTA-monoamide conjugates with precisely controlled nanosizes for magnetic resonance angiography. Biomacromolecules.